# 3'-Aza-2'-[^18^F]fluorofolic acid

Chemical name: | 3'-Aza-2'-[^18^F]fluorofolic acid
Abbreviated name: | 3'-Aza-2'-[^18^F]FFA, [^18^F]6
Synonym:
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Aza%20fluorofolic%20acid)]

Folic acid is a water-soluble B vitamin (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Epithelial cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a receptor on the cell membrane with higher affinity for folate (dissociation constant (K_d_) = 0.5 nM), which allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells have been found to overexpress the folate receptor (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the corresponding normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have also been found to have the folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate (http://www.ncbi.nlm.nih.gov/books/NBK23699/), ^99m^Tc-EC-folate (http://www.ncbi.nlm.nih.gov/books/NBK23152/), and ^68/67/66^Ga-γ-DF-folate (http://www.ncbi.nlm.nih.gov/books/NBK23092/)) have been studied in tumor imaging (4-7). Bettio et al. (8) reported the synthesis of ^18^F-labeled folate by reaction of [^18^F]4-fluorobenzylamine (FBA) with the α- and γ-carboxyl groups of folic acid. [^18^F]α/γ-FBA-folate (http://www.ncbi.nlm.nih.gov/books/NBK23020/) has been evaluated as a positron emission tomography (PET) agent for detection of folate receptors in tumors in mice. Ross et al. (9) introduced the ^18^F radiolabel at the 2' position of the 4-amino-benzoyl moiety in folic acid to form 2'-[^18^F]fluorofolic acid (2'-[^18^F]FFA (http://www.ncbi.nlm.nih.gov/books/NBK53270/)). 2'-[^18^F]FFA was found to be a specific, high-affinity PET agent for imaging folate receptor-positive tumors in mice. However, the low radiochemical yield (1%–4%) from multistep radiosynthesis limited its routine clinical use. Betzel et al. (10) replaced the phenyl ring in 2'-[^18^F]FFA with a pyridine ring to produce 3'-Aza-2'-[^18^F]fluorofolic acid (3'-Aza-2'-[^18^F]FFA or [^18^F]6) for use with PET imaging of folate receptor in nude mice bearing human nasopharyngeal carcinoma KB tumors.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (folate receptors (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Aza%20fluorofolic%20acid%20and%20synthesis)]

Betzel et al. (10) prepared 3'-Aza-2'-[^18^F]FFA with a two-step synthesis using a standard nucleophilic radiofluorination ([^18^F]KF/Kryptofix 2.2.2) reaction of N^3^-acetyl-3'-aza-2'-chlorofolic acid di-tert-butylester (160ºC, 10 min) and subsequent acid hydrolysis (60ºC, 10 min). Maximal overall radiochemical yield was 9%, with >98% radiochemical purity. The total synthesis time was 110 min, and the specific activity was 35–127 GBq/µmol (0.95–3.43 mCi/µmol) at the end of synthesis. 3'-Aza-2'-[^18^F]FFA is hydrophilic, with a logD_7.4_ value of −4.2 ± 0.1. 3'-Aza-2'-[^18^F]FFA was found to be stable in human blood plasma for 4 h at 37°C, and no defluororination was observed after 1 h of incubation with glutathione and human liver S9-fraction at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Aza%20fluorofolic%20acid%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB cell line expresses the folate receptor as determined with [^3^H]folate-binding studies in cultures (8). The mean 50% inhibition (IC_50_) concentrations for 3'-Aza-2'-FFA, 2'-FFA, and folic acid were 1.4 ± 0.5, 0.9 ± 0.1, and 1.1 ± 0.4 nM (10), respectively. Therefore, 3'-Aza-2'-FFA has a binding affinity to folate receptor comparable to that of native folic acid and 2'-FFA. 3'-Aza-2'-[^18^F]FFA exhibited ~78% accumulation of added radioactivity, and ~19% was internalized after incubation for 2 h at 37°C with KB cells. Co-incubation with excess folic acid inhibited the radioactivity accumulation by >98%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Aza%20fluorofolic%20acid%20and%20rodentia)]

Betzel et al. (10) performed ex vivo biodistribution studies of 5 MBq (0.14 mCi) 3'-Aza-2'-[^18^F]FFA in nude mice (n = 4/group) bearing KB tumor xenografts at 30, 60, and 90 min after intravenous injection. Tumor accumulation was 11.70 ± 0.87% injected dose/gram (ID/g) at 30 min, 11.86 ± 1.73% ID/g at 60 min, and 12.59 ± 1.77% ID/g at 90 min. The tumor accumulation of 3'-Aza-2'-[^18^F]FFA was higher than that of [^18^F]α/γ-FBA-folate (http://www.ncbi.nlm.nih.gov/books/NBK23020/) (6.65 ± 1.80% ID/g at 125 min) (8) and 2'-[^18^F]FFA (http://www.ncbi.nlm.nih.gov/books/NBK53270/) (9.37 ± 1.76% ID/g at 75 min) (9). The organ with the highest maximum accumulation was the kidneys (57.33% ID/g at 90 min), followed by the salivary glands (14.95% ID/g at 60 min), liver (13.72% ID/g at 60 min), gallbladder (9.26% ID/g at 90 min), and stomach (2.83% ID/g at 60 min). The radioactivity levels in the blood and bone at 60 min were 0.55% ID/g and 1.57% ID/g, respectively. Accumulation levels in the brain, lungs, heart, spleen, and intestine were <2% ID/g. No radioactive metabolites were detected in the blood, urine, and tumor at 30 min after injection. The tumor/blood ratios were 11.1, 21.6, and 23.8 at 30, 60, and 90 min, respectively. Pretreatment with folic acid (200 μg/mouse) 10 min before 3'-Aza-2'-[^18^F]FFA injection reduced radioactivity accumulation at 60 min by 96% in the salivary glands, 85% in the tumors, and 89% in the kidneys. Less reduction was observed in the lungs, heart, spleen, bone, muscle, and stomach. No reduction was observed in the gallbladder, intestine, and liver.

The whole-body distribution of 13 MBq (35 mCi) 3'-Aza-2'-[^18^F]FFA was also assessed with PET imaging at 120–150 min after injection (10). High accumulation was visualized in the kidneys, salivary glands, gallbladder, urinary bladder, tumors, and liver. The accumulation of radioactivity in the tumors, salivary glands, and kidneys was reduced to near background level after folic acid pretreatment.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Aza%20fluorofolic%20acid%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Aza%20fluorofolic%20acid%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Aza%20fluorofolic%20acid%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.
9 Ross T.L., Honer M., Muller C., Groehn V., Schibli R., Ametamey S.M. (2010). A new 18F-labeled folic acid derivative with improved properties for the PET imaging of folate receptor-positive tumors. J Nucl Med.
10 Betzel T., Muller C., Groehn V., Muller A., Reber J., Fischer C.R., Kramer S.D., Schibli R., Ametamey S.M. (2013). Radiosynthesis and Preclinical Evaluation of 3'-Aza-2'-[(18)F]fluorofolic Acid: A Novel PET Radiotracer for Folate Receptor Targeting. Bioconjug Chem.